# [^111^In]-Ethylenedicysteine-murine anti-phosphotyrosine antibody

Chemical name: | [^111^In]-Ethylenedicysteine-murine anti-phosphotyrosine antibody
Abbreviated name: | ^111^In-EC-APT
Synonym:
Agent Category: | Antibody
Target: | Bcr-Abl tyrosine kinase
Target Category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - Rodents | Click here for the nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=Nucleotide&dopt=GenBank&val=33318779) and protein (http://www.ncbi.nlm.nih.gov/sites/entrez?dopt=GenPept&cmd=Retrieve&db=protein&list_uids=148673890) sequence of mouse (Mus musculus) tyrosine kinase.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Bcr+Abl+tyrosine+kinase)]

The overexpression or constitutive activation of non-receptor tyrosine kinase (TK) such as Src- and Bcr-Abl is one of the several mechanisms known to initiate and participate in the progression and metastasis of cancer (1, 2). Because of their role in the development of different neoplasms, small-molecule drugs such as imatinib, dasatinib, and others that block TK activity by inhibiting ATP binding to the enzyme are often used to treat patients suffering from this disease (3, 4). Because several different TK blockers are either under development or are being evaluated in clinical trials (http://clinicaltrials.gov/ct2/results?term=tyrosine+kinase+inhibitors) to treat cancers, it is important to be able to screen patients to determine which TK inhibitor is likely to result in a good prognosis for an individual (5). Although invasive procedures such as biopsies are routinely used to determine the efficacy of an anti-cancer treatment, a noninvasive technique such as imaging would probably be preferred to evaluate drug activity during early stages of the treatment.

Wu et al. envisioned that antibodies labeled with a radionuclide and directed toward an intracellular non-receptor TK could be used for the noninvasive determination of drug efficacy (5). The investigators evaluated an ethylenedicysteine (EC)-murine anti-phosphotyrosine (APT) antibody labeled with radioactive indium (^111^In) (^111^In-EC-APT) to image the Bcr-Abl TK, which is known to be upregulated and to promote chronic myeloid leukemia (6), in a mouse xenograft tumor model. The radiolabeled antibody (Ab) was also used to investigate tumor imaging changes in the animals after treatment with imatinib.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=labeled+Bcr+Abl+anti+tyrosine+kinase+antibody+synthesis)]

The synthesis of ^111^In-EC-APT was described in detail by Wu et al. (5). The various biological reagents used for the studies and described in this chapter, including the control (anti-phospho-Bcr-Abl Ab) and the murine APT 4G10 Abs, were obtained from commercial sources. EC was conjugated to the APT Ab, murine immunoglobulin G_1_ (IgG_1_), anti-phospho-Bcr-Abl Ab, and bovine serum albumin (BSA) with sulfo-N-hydroxysuccinimide (NHS) and 1-ethyl-3-(3-dimethylaminopropyl) carbodiimide hydrochloride (EDC) as the coupling agents.

For the conjugation of EC, the various bioreagents were respectively incubated with a mixture of EC, NHS, and EDC for 17 h at room temperature. The purification and final percent yield of the respective EC-conjugated bioreagents and the ratio of chelating agent per antibody molecule were not reported. For labeling with ^111^In, the radionuclide was mixed with the respective EC-conjugated bioreagent to obtain ^111^In-EC-BSA, ^111^In-EC-IgG_1_, ^111^In-EC-Bcr-Abl, and ^111^In-EC-APT. Purification of the radiolabeled bioreagents was not reported. Radiochemical purity of the ^111^In-labeled biochemicals was reported to be >95%, as determined with thin-layer chromatography. The specific activity and stability of the various labeled bioreagents were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+EC+APT+Rodentia)]

Tumor imaging studies were performed with immunodeficient mice bearing K562 cell tumors, a human chronic myeloid leukemia cell line that constitutively expresses activated Bcr-Abl TK (5). The mice were divided into five groups, each consisting of five animals. The first group received ^111^In-EC-BSA to visualize normal blood flow in the tumor; the second group received ^111^In-EC-APT to determine tumor specificity of the labeled Ab, and the third group was treated with imatinib for 3 days before the ^111^In-EC-APT injection and during the imaging study (a total of 4 or 5 d). Two other groups of animals received either ^111^In-EC-IgG_1_ or ^111^In-EC-Bcr-Abl to serve as the negative and positive controls, respectively. Images were acquired at various time points up to 48 h after the radiobiochemical injection.

Determination of the tumor/non-tumor count densities after planar scintigraphy revealed that there was an increased uptake of ^111^In-EC-APT by the tumors compared with ^111^In-EC-BSA (5). Mice treated with imatinib showed a reduced (P < 0.05) ^111^In-EC-APT uptake. At 48 h after treatment with the radiotracers, one animal from each group was subjected to single-photon emission computed tomography-computed tomography (SPECT-CT), which produces a dynamic image (for details see Wu et al. (5)) of the combined functional and structural features of the tumor, to measure the precise phosphorylation status of the tumors. Results obtained with SPECT-CT were similar to those obtained with planar scintigraphy. The tumor/normal muscle count ratios (TMR) were determined for all radiotracers used to treat the animals (5). The TMR ratios were reported to be 1.5, 1.9, 4.0, and 6.0 for ^111^In-EC-BSA (used to visualize blood flow), ^111^In-EC-IgG_1_ (negative control), ^111^In-EC-APT, and ^111^In-EC-Bcl-Abl (positive control), respectively.

With results obtained from this study (5), the investigators concluded that imaging could be used to select a specific TK inhibitor for the treatment of certain cancer and to predict the treatment response in a clinical setting (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+EC+APT+Non+Primate+Mammal+studies)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+EC+APT+Non+Human+Primate+studies)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+EC+APT+Human+studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Finn R.S. (2008). Targeting Src in breast cancer. Ann Oncol.
2 Pytel D., Sliwinski T., Poplawski T., Ferriola D., Majsterek I. (2009). Tyrosine kinase blockers: new hope for successful cancer therapy. Anticancer Agents Med Chem.
3 Muller B.A. (2009). Imatinib and its successors--how modern chemistry has changed drug development. Curr Pharm Des.
4 Gora-Tybor J., Robak T. (2008). Targeted drugs in chronic myeloid leukemia. Curr Med Chem.
5 Wu, J.Y., D.J. Yang, L.S. Angelo, S. Kohanim, and R. Kurzrock, Molecular imaging of Bcr-Abl phosphokinase in a xenograft model. Mol Cancer Ther, 2009
6 O'Hare T., Deininger M.W. (2008). Toward a cure for chronic myeloid leukemia. Clin Cancer Res.